# Thermally cross-linked superparamagnetic iron oxide nanoparticle-A10 RNA aptamer-doxorubicin conjugate

Chemical name: | Thermally cross-linked superparamagnetic iron oxide nanoparticle-A10 RNA aptamer-doxorubicin conjugate
Abbreviated name: | TCL-SPION-Apt(Dox)
Synonym:
Agent category: | Nucleic acid (nanoparticle)
Target: | Prostate-specific membrane antigen (PSMA)
Target category: | Nucleic acid binding protein
Method of detection: | Magnetic resonance imaging (MRI), optical imaging
Source of signal/contrast: | Iron oxides, doxorubicin-RNA complex
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TCL+SPION + Apt + Dox)]

Prostate-specific membrane antigen (PSMA) is a type II membrane glycoprotein with a molecular weight of ~100 kDa (1). PSMA is composed of several domains, including a potential phosphorylation site in the cytoplasmic tail (amino acids 1–18), a highly hydrophobic α-helix in the transmembrane region (amino acids 19–43), and catalytic sites in the extensive extracellular domain (amino acids 44–750). Two unique enzymatic functions are found in PSMA: N-acetylated, α-linked, dipeptidase (NAALADase) activity and folate hydrolase activity. As a prostate cancer cell (PCa) marker, PSMA expression is primarily prostate-specific (~100% in androgen-independent PCa cells), with very low levels (~1,000-fold less) in the brain, salivary glands, and small intestine. Thus, PSMA has become an excellent target for imaging and therapy.

Aptamers (from the Latin aptus, to fit, and the Greek meros, part or region) are single-stranded or double-stranded oligonucleotides (RNA or DNA, respectively) that are modified to bind a variety of targets with high binding affinity and specificity (2). Aptamers range in size from 20 to 80 base pairs (~6–26 kDa) with dissociation constants in the range of 10 pM to 10 nM (3). Unlike linear oligonucleotides, which contain genetic information or antisense oligonucleotides that interrupt the transcription of genetic information, aptamers are globular molecules with a shape similar to tRNA and bind to target proteins specifically (4). A10 RNA aptamer (Apt) is a nuclease-stabilized 2’-fluoropyrimidine RNA molecule of 57 base pairs with a molecular weight of 18.5 kDa (5). Its 2’-fluoro-modified ribose on all pyrimidines and 3’-inverted deoxythymidine cap provide significant resistance to nuclease in blood (6). Apt has a single 5’-CG-3’ sequence in its predicted double-stranded stem region, which is a preferred binding site for the anthracycline class of anticancer drugs such as doxorubicin (Dox) (7). Dox intercalates within the GC pair in Apt to form physical conjugate Apt(Dox) at molar ratio of 1.11:1 (dissociation constant = 600 nM) and emit fluorescence simultaneously. Because Dox possesses high efficacy against a range of neoplasms, including acute lymphoblastic and myeloblastic leukemias, malignant lymphomas, soft tissue and bone sarcomas, and breast, ovarian, prostate bladder, gastric, and bronchogenic carcinomas (8), this complex can be used as a PSMA-specific drug carrier to deliver Dox to PCa.

Superparamagnetic iron oxide nanoparticles (SPION) consist of magnetite (Fe_3_O_4_), which has a high magnetic susceptibility to induce a significant magnetization inside a magnetic field. The resulting microscopic field gradients diphase nearby protons and cause a reduction of T_2_ relaxation times (9). SPION readily forms aggregates as a result of nonspecific adsorption of plasma protein in blood, and SPION is cleared rapidly from the body by functions of the reticular endothelial system (RES) such as via macrophages (10). Coating the surface of SPION with a protein-repelling polymer layer such as poly(ethyleneglycol) (PEG) can prevent the absorption of plasma proteins or cells onto the surface of SPION (11). The coating can be conducted via surface trialkoxysilane as an anchor part (12). For example, poly(3-trimethoxysilyl)propyl methacrylate-r-PEG methyl ether methacrylate) (poly(TMSMA-r-PEGMA)) is a PEG-silane copolymer consisting of surface-reactive Si(OMe)_3_ groups and protein-repelling PEG chains (11). This coating becomes highly stabilized by simple heat treatment through condensation of hydrolyzed silane group (Si(OH)_3_) to form a thermally cross-linked (TCL) polymer.

TCL-SPION-A10 RNA aptamer-doxorubicin conjugate (TCL-SPION-Apt(Dox)) is a PSMA-specific agent used for magnetic resonance imaging the delivery of the anticancer drug Dox (13). TCL-SPION-Apt(Dox) contains three components: a PSMA-specific RNA aptamer A10 (Apt) covalently attached to the core surface as a targeting molecule and drug carrier, an anthracycline class of anticancer drug Dox as chemotherapeutic agent and optical sensor, and a TCL-SPION coated with a TCL carboxylic acid-PEG-silane copolymer as a magnetic resonance contrast agent and as a carrier for Apt(Dox). The PEGylated surface prevents protein and cell adsorption, while the carboxyl groups allow for conjugation of targeting moieties such as Apt. TCL-SPION-Apt(Dox) can be used to image the drug delivery to PCas.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(TCL+SPION + Apt + Dox)+AND+synthesis%0D%0A)]

The preparation of TCL-SPION-Apt(Dox) was conducted in several steps (11, 13). First, N-acryloxysuccinimide (NAS), 3-(trimethoxysilyl)propyl methacrylate (TMSMA), and PEG-methyl ether methacrylate (PEGMA; molecular weight ~475) were mixed at a molar ratio of 1:1:0.86 (11). After degassing with N_2_ for 15 min, 2,2’-azo-bis-isobutyronitrile was added for 24 h at 70ºC to initiate a free radical polymerization. The produced poly(TMSMA-r-PEGMA-r-NAS) (26.795 kDa) possessed a polydispersity of 1.646. Poly(TMSMA-r-pPEGMA-r-NAS) was further hydrolyzed to convert its trimethoxysilane and N-hydroxysuccinimide (NHS) ester into trihydroxysilane and carboxylic acid, respectively. Second, freshly prepared magnetite (Fe_3_O_4_) was reacted with the hydrolyzed form of poly(TMSMA-r-PEGMA-r-NSA) followed by thermal cross-linking for 2 h at 80ºC. The produced TCL-SPION, with carboxyl groups as the surface functional groups (carboxyl-TCL-SPION), was then treated with N-(3-dimethylaminopropyl)-N’-ethylcarbodiimide and NHS (13). Commercially available N-terminated A10 aptamer (57 base pairs) was added 15 min later and reacted for 4 h to produce TCL-SPION-Apt, in which the molar ratio of PEG, Si(OCH_3_)_3_, and NHS-activated carboxylic acid was determined with ^1^H nuclear magnetic resonance imaging to be 1:0.85:0.71. Finally, unreacted Apt was removed and Dox was loaded to TCL-SPION-Apt to form the intercalated conjugate TCL-SPION-Apt(Dox). The molecular sizes were 60.8 ± 1.9 nm for TCL-SPION and 66.4 ± 1.5 nm for TCL-SPION-Apt.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(TCL+ SPION + Apt + Dox)+AND+%22in+vitro%22)]

Wang et al. studied the in vitro cellular uptake of TCL-SPION-Apt (13). PSMA-expressing PCa cells (LNCaP) and non-PSMA-expressing PCa cells (PC3) were incubated with 0.1 mg/ml TCL-SPION-Apt at 37ºC at time intervals of 1, 3, 6, 12, 18, and 24 h and followed by Prussian blue staining. The uptake of TCL-SPION-Apt in LNCaP cells was found as early as 3 h and gradually increased in a time-dependent manner, whereas no apparent cellular uptake was observed in PC3 cells. This result demonstrated differential targeting of PSMA-expressing PCa cells by TCL-SPION-Apt. The alteration of relaxation times (T_1_, T_2_) caused by cellular uptake of TCL-SPION-Apt was examined with nuclear magnetic resonance measurement (13). LNCap cells and PC3 cells were incubated for 6 h with TCL-SPION-Apt. A dramatic decrease was found only in the LNCaP cells, in which T_1_ decreased from 1,939 ± 116 to 263 ± 23 ms and T_2_ decreased from 104 ± 1.4 to 26.6 ± 0.4 ms. As a control, LNCap cells and PC3 cells were also incubated with non-targeted TCL-SPION for 6 h. Only a small alteration was observed in the LNCaP cells in that T_1_ decreased slightly from 1,939 ± 116 to 1,521 ± 201 ms and T_2_ decreased 104 ± 1.4 to 89.8 ± 1.1 ms. These data exhibited a high sensitivity in detecting PSMA-expressing PCa cells. The effect of TCL-SPION-Apt(Dox) on cellular proliferation was examined in vitro (13). After incubation with TCL-SPION-Apt(Dox) (0.1 mg/ml intercalated with 5 μM Dox) for 3 h, the viability was evaluated with methylthiazole tetrazolium (MTT) assay, which was 47.3 ± 1.4% for LNCaP cells and 69.3 ± 1.7% for PC3 cells. The free Dox was shown to be equipotent against both LNCaP and PC3 cell lines.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(TCL+ SPION + Apt + Dox) +AND++rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(TCL+ SPION + Apt + Dox) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(TCL+ SPION + Apt + Dox) +AND+human)]

No publication is currently available.

### NIH Support

CA 119349, EB 03647

## References

1 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
2 Ng E.W., Shima D.T., Calias P., Cunningham E.T., Guyer D.R., Adamis A.P. (2006). Pegaptanib, a targeted anti-VEGF aptamer for ocular vascular disease. Nat Rev Drug Discov.
3 Levy-Nissenbaum E., Radovic-Moreno A.F., Wang A.Z., Langer R., Farokhzad O.C. (2008). Nanotechnology and aptamers: applications in drug delivery. Trends Biotechnol.
4 Hicke B.J., Stephens A.W. (2000). Escort aptamers: a delivery service for diagnosis and therapy. J Clin Invest.
5 Lupold S.E., Hicke B.J., Lin Y., Coffey D.S. (2002). Identification and characterization of nuclease-stabilized RNA molecules that bind human prostate cancer cells via the prostate-specific membrane antigen. Cancer Res.
6 Farokhzad O.C., Jon S., Khademhosseini A., Tran T.N., Lavan D.A., Langer R. (2004). Nanoparticle-aptamer bioconjugates: a new approach for targeting prostate cancer cells. Cancer Res.
7 Zhang L., Radovic-Moreno A.F., Alexis F., Gu F.X., Basto P.A., Bagalkot V., Jon S., Langer R.S., Farokhzad O.C. (2007). Co-delivery of hydrophobic and hydrophilic drugs from nanoparticle-aptamer bioconjugates. ChemMedChem.
8 Bagalkot V., Farokhzad O.C., Langer R., Jon S. (2006). An aptamer-doxorubicin physical conjugate as a novel targeted drug-delivery platform. Angew Chem Int Ed Engl.
9 Bulte J.W., Brooks R.A., Moskowitz B.M., Bryant L.H., Frank J.A. (1998). T1 and T2 relaxometry of monocrystalline iron oxide nanoparticles (MION-46L): theory and experiment. Acad Radiol.
10 Lee H., Lee E. (2006). K. Kim do, N.K. Jang, Y.Y. Jeong, and S. Jon, Antibiofouling polymer-coated superparamagnetic iron oxide nanoparticles as potential magnetic resonance contrast agents for in vivo cancer imaging. J Am Chem Soc.
11 Lee H., Yu M.K., Park S., Moon S., Min J.J., Jeong Y.Y., Kang H.W., Jon S. (2007). Thermally cross-linked superparamagnetic iron oxide nanoparticles: synthesis and application as a dual imaging probe for cancer in vivo. J Am Chem Soc.
12 Jon S., Seong J., Khademhosseini A., Tran T.N.T., Laibinis P.E., Langer R. (2003). Constructtion of Nonbiofouling surfaces by polymeric self-aassembled monolayers. Langmuir.
13 Wang, A.Z., V. Bagalkot, C.C. Vasilliou, F. Gu, F. Alexis, L. Zhang, M. Shaikh, K. Yuet, M.J. Cima, R. Langer, P.W. Kantoff, N.H. Bander, S. Jon, and O.C. Farokhzad, Superparamagnetic Iron Oxide Nanoparticle-Aptamer Bioconjugates for Combined Prostate Cancer Imaging and Therapy. ChemMedChem, 2008